# VivoTag-S 750-(S)-2-amino-4-pentynoic acid^12^-exendin-4

Chemical name: | VivoTag-S 750-(S)-2-amino-4-pentynoic acid^12^-exendin-4
Abbreviated name: | E4_X12_-VT750
Synonym:
Agent category: | Peptide
Target: | Glucagon-like peptide-1 receptor (GLP-1R)
Target category: | Receptor
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | VivoTag-S 750 (VT750)
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=248418), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&val=1916066) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=14526) for more information about exendin-4.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VT750%20Exendin-4)]

Glucagon-like peptide-1 (GLP-1; 30 amino acids) is secreted from enteroendocrine cells of the distal small intestine in response to food ingestion (1). GLP-1 plays an important role in glucose metabolism and homeostasis by inhibiting gastric emptying, glucagon secretion, and glucose production (2). In addition, GLP-1 induces insulin release from the pancreatic β-cells as well as their proliferation. The GLP-1 receptor (GLP-1R) has been identified in normal tissues such as the pancreatic β-cells, stomach, brain, and lung, and it has been shown to be highly overexpressed in human insulinomas and gastrinomas (3). In insulinomas, GLP-1R density is considerably greater, and the GLP-1R is more frequently observed than somatostatin receptors.

Exendin-4 is a GLP-1 analog with 39 amino acids isolated from the venom of the Gila monster (Heloderma suspectum) (4). Exendin-4 and GLP-1 share a 53% amino acid sequence homology. Exendin-4 is a more potent and longer-lasting GLP-1R agonist than GLP-1. Exendin-4 is resistant to cleavage by dipeptidyl peptidase IV, whereas the first two N-terminal amino acids of GLP-1 are rapidly cleaved. Exenatide, a synthetic version of exendin-4, is the first GLP-1 mimetic approved by the United States Food and Drug Administration (FDA) for use in select patients with type 2 diabetes (5). ^111^In-Labeled diethylenetriamine pentaacetic acid-aminohexanoic acid-Lys^40^-exendin-4 (^111^In-DTPA-Ahx-Lys^40^-exendin-4) has been developed for single-photon emission computed tomography (SPECT) imaging of the GLP-1R (6).

For optical near-infrared (NIR) fluorescence imaging, Reiner et al. (7) replaced the Lys at position 12 of exendin-4 with the non-natural amino acid (S)-2-amino-4-pentynoic acid to form a neopeptide, E4_X12_. The azide-functionalized NIR dye VivoTag-S 750 (VT750) was conjugated to the non-natural amino acid at position 12 via azide-alkyne cycoaddition to form VT750-(S)-2-amino-4-pentynoic acid^12^-exendin-4 (E4_X12_-VT750). E4_X12_-VT750 has been evaluated as an optical imaging agent for GLP-1R density and β-cell mass (BCM) in normal mice and in mice treated with streptozotocin (STZ) to induce BCM loss and diabetes.

### Related Resource Links:

- Chapters in MICAD (GLP-1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=GLP-1R%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (GLP-1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=2740%5Buid%5D)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (GLP-1R (http://omim.org/entry/138032))
- Clinical trials (Exendin (http://www.clinicaltrials.gov/ct2/results?term=exendin))
- Drug information in FDA (Exendin (http://google2.fda.gov/search?q=exendin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VT750%20Exendin-4%20and%20synthesis)]

11-Azido-3,6,9-trioxaundecan-1-amide-VT750 (azido-VT750) was prepared by incubation of 11-azido-3,6,9-trioxaundecan-1-amine (46 µmol) and VT750 (8.6 µmol) for 3 h at room temperature (7). Azido-VT750 was purified with high-performance liquid chromatography (HPLC), with a chemical yield of 36%. Azido-VT750 (1.2 µmol) was added to an aqueous solution (pH 7.2) of E4_X12_ (0.8 µmol), ascorbic acid (2.5 mmol), and CuSO_4_ (2.5 mmol). The mixture was incubated for 18–20 h at room temperature. E4_X12_-VT750 was isolated with HPLC, with a chemical yield of 64%. E4_X12_-VT750 was identified with HPLC and matrix-assisted laser desorption-ionization mass spectrometry (MALDI-MS). There was one VT750 dye per conjugate. E4_X12_-VT750 exhibited an absorption maximum at 754 nm and an emission maximum of 774 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VT750%20Exendin-4%20and%20in%20vitro)]

Cellular accumulation of E4_X12_-VT750 (0, 0.01, 0.1, 1, 10, and 100 nM) was measured in mouse insulinoma MIN6 (GLP-1R–positive), HEK/hGLP-1R (human GLP-1R–positive), and NIH3T3 fibroblast (GLP-1R–negative) cell lines (7). There was a dose-dependent increase in cellular fluorescence signals in MIN6 and HEK/hGLP-1R cells with a 50% effective dose of 3.3 nM in both cell lines for 90 min at 37°C. However, no signal was observed in NIH3T3 cells, even at 100 nM of E4_X12_-VT750. Preincubation with various concentrations of exendin-4 for 60 min before the addition of 10 nM E4_X12_-VT750 decreased the fluorescence signals in MIN6 and HEK/hGLP-1R cells with a 50% inhibition concentration of ~3 nM. Fluorescence microscopy showed that E4_X12_-VT750 was internalized into the vesicular compartments of HEK/hGLP-1R cells. The cell-surface binding and internalization of E4_X12_-VT750 were inhibited with excess exendin-4.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VT750%20Exendin-4%20and%20rodentia)]

Reiner et al. (7) performed intravital confocal imaging of pancreatic islets and β-cells in mice with the mouse insulin 1 promoter green fluorescence protein (MIP-GFP). NIR fluorescence signal was observed in β-cells within 10 min after intravenous injection of 2–4 nmol E4_X12_-VT750, and the signal gradually increased to ~64-fold more than background at 120 min. Injection of exendin-4 (15 nmol) 20 min before injection of E4_X12_-VT750 reduced the signal to background level in β-cells at 60 min after injection. E4_X12_-VT750 exhibited a weighted blood half-life of 84 s. E4_X12_-VT750 fluorescence signal colocalized with GFP signal in β-cells (R^2^ = 0.944). NIR fluorescence signal was also observed with microendoscopic imaging of the pancreata of anesthetized mice. Ex vivo NIR fluorescence distribution in organs of normal mice at 60 min after E4_X12_-VT750 injection was compared with the autofluorescence of noninjected mice. The organ with the highest fluorescence was the kidney (69%), followed by the liver (15%), pancreas (8%), intestine (4%), lung (3%), stomach (2%), spleen (<1%), and heart (<1%). E4_X12_-VT750 was mostly eliminated by the kidneys and liver.

Ex vivo studies of pancreatic accumulation of E4_X12_-VT750 were performed in normal mice (n = 4–5/group) treated with various doses (0, 75, 150, and 500 mg/kg) of STZ to induce BCM loss and diabetes. Pancreatic fluorescence signal was obtained as fluorescence/volume, and BCM was determined with histo-immunological staining of pancreas sections at 60 min after injection. Mice exhibited normal glucose levels with 75 mg/kg STZ and became hyperglycemic with 150 and 500 mg/kg STZ. There was a dose-dependent loss of NIR fluorescence signals in the pancreata from the STZ-treated mice. There was a good correlation (R^2^ = 0.854, P < 0.0001) between loss of fluorescence signal and BCM.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VT750%20Exendin-4%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VT750%20Exendin-4%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VT750%20Exendin-4%20and%20human)]

No publication is currently available.

## NIH Support

P01 AI54904, U24 CA092782, R01 67536, R01 EB006432, IRL9 EB0083539-01, KL2 RR025757

## References

1 Theodorakis M.J., Carlson O., Michopoulos S., Doyle M.E., Juhaszova M., Petraki K., Egan J.M. (2006). Human duodenal enteroendocrine cells: source of both incretin peptides, GLP-1 and GIP. Am J Physiol Endocrinol Metab.
2 Doyle M.E., Egan J.M. (2001). Glucagon-like peptide-1. Recent Prog Horm Res.
3 Reubi J.C., Waser B. (2003). Concomitant expression of several peptide receptors in neuroendocrine tumours: molecular basis for in vivo multireceptor tumour targeting. Eur J Nucl Med Mol Imaging.
4 Meier J.J., Nauck M.A. (2005). Glucagon-like peptide 1(GLP-1) in biology and pathology. Diabetes Metab Res Rev.
5 Nielsen L.L., Young A.A., Parkes D.G. (2004). Pharmacology of exenatide (synthetic exendin-4): a potential therapeutic for improved glycemic control of type 2 diabetes. Regul Pept.
6 Gotthardt M., Lalyko G., van Eerd-Vismale J., Keil B., Schurrat T., Hower M., Laverman P., Behr T.M., Boerman O.C., Goke B., Behe M. (2006). A new technique for in vivo imaging of specific GLP-1 binding sites: First results in small rodents. Regul Pept.
7 Reiner T., Thurber G., Gaglia J., Vinegoni C., Liew C.W., Upadhyay R., Kohler R.H., Li L., Kulkarni R.N., Benoist C., Mathis D., Weissleder R. (2011). Accurate measurement of pancreatic islet beta-cell mass using a second-generation fluorescent exendin-4 analog. Proc Natl Acad Sci U S A.